# (-)-7-Methyl-2-exo-[3'-(6-[^18^F]fluoropyridin-2-yl)-5'-pyridinyl]-7-azabicyclo[2.2.1]heptane

Chemical name: | (-)-7-Methyl-2-exo-[3'-(6-[^18^F]fluoropyridin-2-yl)-5'-pyridinyl]-7-azabicyclo[2.2.1]heptane
Abbreviated name: | [^18^F](-)-6c
Synonym:
Agent category: | Compound
Target: | Neuronal α4β2 nicotinic acetylcholine receptor (nAChR)
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Other Non-primate Mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=nAchR%20(-)-6c)]

Neuronal α4β2 nicotinic cholinergic receptors (nAChRs) are part of a heterogeneous family of ligand-gated ion channels expressed in the central nervous system, where their activation by acetylcholine and nicotine causes a rapid increase in cellular permeability to ions, such as Na^+^ and Ca^2+^ (1-3). Nicotinic receptors exist as pentamers (homomeric or heteromeric) in various brain regions and ganglia. There are nine subtypes of ligand-binding α receptors (α2 to α10) and four subtypes of structural β receptors (β2 to β5). nAChRs have been found to be involved in cognitive processes such as learning memory and control of movement in normal subjects. nAChR dysfunction has been implicated in a number of human diseases such as schizophrenia, Huntington's disease, Alzheimer's disease, and Parkinson's disease. nAChRs also play a significant role in nicotine addiction and other health problems associated with tobacco smoking.

3-[2(S)-2-Azetidinylmethoxy]pyridine (A-85380) is a highly potent and selective α4β2 nAChR agonist with subnanomolar affinity (4, 5). 6-[^18^F]Fluoro-A-85380 and 2-[^18^F]fluoro-A-85380 have been studied in humans as positron emission tomography (PET) agents for α4β2 nAChR imaging in the brain. A-85380 has also been labeled as 5-[^123^I]iodo-3-[2(S)-2-azetidinylmethoxy]pyridine (5-[^123^I]iodo-A-85380 (5-[^123^I]IA)), which has been developed as a single-photon emission computed tomography (SPECT) agent for the non-invasive study of α4β2 nAChR in the brain. However, prolonged imaging times (>5 h) are required for reliable quantification because of the slow kinetics of this agent. (-)-7-Methyl-2-exo-[3'-(6-fluoropyridin-2-yl)-5'-pyridinyl]-7-azabicyclo[2.2.1]heptanes ((-)-6c) has been shown to be a potent and selective α4β2 nAChR competitive antagonist for α4β2 nAChR with subnanomolar affinity (6). [^18^F](-)-6c is being developed as a PET agent for the noninvasive study of α4β2 nAChR in the brain.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=nAchR%20(-)-6c%20and%20synthesis)]

Gao et al. (6) reported synthesis of [^18^F](-)-6c by the standard ([^18^F]KF/Kryptofix 2.2.2) ^18^F-nucleophilic aromatic fluorination of 7-Methyl-2-exo-[3'-(6-bromopyridin-2-yl)-5'-pyridinyl]-7-azabicyclo[2.2.1]heptane at 180ºC for 18 min. [^18^F](-)-6c was purified with high-performance liquid chromatography (HPLC). Average radiochemical yield was 34 ± 13% (nondecay-corrected, based on [^18^F]KF) at the end of synthesis. The radiochemical purity was >98% with specific activities of 692 ± 170 GBq/µmol (18.7 ± 4.6 Ci/µmol, n = 4) at the end of synthesis. The enantiomeric purity of [^18^F](−)-6c (>99%) was determined by chiral HPLC. The total synthesis time was 60 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=nAchR%20(-)-6c%20and%20in%20vitro)]

Gao et al. (6) reported that (-)-6c exhibited inhibition constant (K_i_) values of 0.26, 7.8 and 310 nM in human α4β2, α2β4, and α3β4 receptors, respectively. On the other hand, 2-fluoro-A-85380 exhibited K_i_ values of 1.33, 181, and 3,680 nM in human α4β2, α2β4, and α3β4 receptors, respectively. The lipophilicity (log P) values of (-)-6c and 2-fluoro-A-85380 were 0.99 and -1.43, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=nAchR%20(-)-6c%20and%20rodentia)]

Gao et al. (6) reported biodistribution studies of ~1.5 MBq (~0.04 mCi) [^18^F](-)-6c in mice (n = 3/group), showing peak accumulation in the thalamus, frontal cortex and cerebellum of 14%, 8% and 4% injected dose/gram (ID/g) at 5 min, respectively. The washout rate from the cerebellum was faster than that from all other regions measured, providing the thalamus/cerebellum ratio of 12 at 60 min after injection. Pretreatment of cytisine (5 mg/kg, s.c) or (-)-6c (20 nmol/kg) reduced the radioactivity in the thalamus and frontal cortex by 70-94% with marginal inhibition in the cerebellum. The fraction of unchanged [^18^F](-)6c in the plasma and brain determined with HPLC was 12.3% and 92.5% at 60 min after injection, respectively. Three major hydrophilic metabolites were found in the blood at 30 min after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=nAchR%20(-)-6c%20and%20(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=nAchR%20(-)-6c%20and%20(primate%20not%20human))]

[^18^F](-)-6c PET studies with baboons showed substantial brain accumulation with selective maximal uptake in the regions of the thalamus, intermediate uptake in the cortex and basal ganglia in 7-28 min after injection (6). The cerebellum showed lower binding than the other brain regions, whereas it exhibited faster washout rate than that from all other regions measured. [^18^F](-)-6c radioactivity was reduced to background level of cerebellum by cytisine pretreatment. PET modeling using constrained and nonconstrained k_4_-models demonstrated that 90−100 min of scanning time was required for estimation of both the volume of distribution and binding potential in all regions in the baboon brain. On the other hand, >6 h of scanning time was required for PET quantification of 2-[^18^F]fluoro-A85380. The fraction of unchanged [^18^F](-)-6c in the plasma determined with HPLC was 14.9% at 60 min after injection. One major and two minor hydrophilic metabolites were found.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=nAchR%20(-)-6c%20and%20human)]

No publication is currently available.

## NIH Support

MH079017, MH32004

## References

1 Alkondon M., Albuquerque E.X. (2004). The nicotinic acetylcholine receptor subtypes and their function in the hippocampus and cerebral cortex. Prog Brain Res.
2 Gotti C., Riganti L., Vailati S., Clementi F. (2006). Brain neuronal nicotinic receptors as new targets for drug discovery. Curr Pharm Des.
3 Hogg R.C., Raggenbass M., Bertrand D. (2003). Nicotinic acetylcholine receptors: from structure to brain function. Rev Physiol Biochem Pharmacol.
4 Abreo M.A., Lin N.H., Garvey D.S., Gunn D.E., Hettinger A.M., Wasicak J.T., Pavlik P.A., Martin Y.C., Donnelly-roberts D.L., Anderson D.J., Sullivan J.P., Williams M., Arneric S.P., Holladay M.W. (1996). Novel 3-Pyridyl ethers with subnanomolar affinity for central neuronal nicotinic acetylcholine receptors. J Med Chem.
5 Sullivan J.P., Donnelly-Roberts D., Briggs C.A., Anderson D.J., Gopalakrishnan M., Piattoni-Kaplan M., Campbell J.E., McKenna D.G., Molinari E., Hettinger A.M., Garvey D.S., Wasicak J.T., Holladay M.W., Williams M., Arneric S.P. (1996). A-85380 [3-(2(S)-azetidinylmethoxy) pyridine]: in vitro pharmacological properties of a novel, high affinity alpha 4 beta 2 nicotinic acetylcholine receptor ligand. Neuropharmacology.
6 Gao Y., Kuwabara H., Spivak C.E., Xiao Y., Kellar K., Ravert H.T., Kumar A., Alexander M., Hilton J., Wong D.F., Dannals R.F., Horti A.G. (2008). Discovery of (-)-7-methyl-2-exo-[3'-(6-[18F]fluoropyridin-2-yl)-5'-pyridinyl]-7-azabicy clo[2.2.1]heptane, a radiolabeled antagonist for cerebral nicotinic acetylcholine receptor (alpha4beta2-nAChR) with optimal positron emission tomography imaging properties. J Med Chem.